# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-D-Tyr-D-Lys(HSG)-D-Glu-D-Lys(HSG)-NH_2_ (IMP-288)

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-D-Tyr-D-Lys(HSG)-D-Glu-D-Lys(HSG)-NH_2_ (IMP-288)
Abbreviated name: | [^111^In]-IMP-288
Synonym:
Agent Category: | Compound
Target: | Anti–histamine-succinyl-glycine (HSG) mAb Fab’ fragment
Target Category: | Antibody
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Pretargeting%20antibodies&cmd=DetailsSearch)]

Most individuals suffering from pancreatic adenocarcinoma (PAC) do not survive for more than 1 year after diagnosis, and <1% of these patients live beyond 5 years (1). Although surgical resection of the cancer is a possible intervention for this disease, only 10%–25% of the patients are considered suitable for this treatment because, by the time that the neoplasm is detected, the malignancy has metastasized to other organs and the tumor load in the patient is too high to warrant surgery (2). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy or a combination of the two; however, these treatments are not curative because they only prolong survival and improve the quality of life of the patient (2). Early detection of this invasive cancer would facilitate proper staging of the disease so that a suitable treatment regimen can be initiated to possibly improve patient prognosis (3).

In this regard, the monoclonal antibody (mAb) PAM4, which specifically targets mucin 1 (MUC1), a glycoprotein that is overexpressed only in PAC tumors, was developed, radiolabeled with ^131^I or ^111^In, and shown with scintigraphy to detect neoplastic tumors in patients with pancreatic malignancies (4). However, intact radiolabeled antibodies (5) are known to have incomplete tumor penetration due to their large size (~150 kDa), and they are of limited utility to visualize cancerous lesions with different imaging modalities because they have a long blood circulating half-life and usually generate a low signal/noise (S/N) ratio (5). To amplify the signal obtained from an imaging agent so that it can be used to detect malignant tumors noninvasively, investigators have developed and evaluated a variety of strategies in preclinical studies with animals. One such strategy involves the pretargeting of cancer lesions with a suitable mAb (or its derivative), allowing some time for the pretargeting Ab to bind to the cancerous tissue and clear from blood circulation; the animals subsequently are injected with an appropriate radiolabeled small molecular weight ligand that binds to the pretargeting mAb or its derivative. This technique has been shown to generate higher S/N ratios during imaging compared to ratios obtained with a directly labeled mAb alone (6-8). Use of the pretargeting technique with multivalent (i.e., containing more than one antigen binding site), multispecific (i.e., can bind more than a single type of antigen) Abs for the imaging and therapy of cancer has been discussed in detail elsewhere (9, 10).

Cardillo et al. developed bsPAM4 (or bsmAb), a divalent, bispecific F(ab’)_2_ mAb, by cross-linking a PAM4 Fab’ fragment to a murine anti–In-diethylenetriamine pentaacetic acid (In-DTPA) mAb Fab’ fragment and used the unlabeled bsPAM4 to pretarget human CaPan-1 cell xenograft PAC tumors in nude mice (4). The animals were then exposed to a radiolabeled peptide hapten that bound to the In-DTPA mAb Fab’; imaging showed that this technique generated higher S/N ratios compared to the directly labeled bsmAb alone. From this study, the investigators concluded that the peptide was suitable for use with scintigraphy to target and visualize human xenograft PAC tumors in nude mice (4). In an effort to further improve the S/N ratio that can be obtained with the pretargeting technique, Gold et al. generated a recombinant trivalent (i.e., three binding sites) bsmAb, designated TF10, and evaluated its use with scintigraphy for the visualization of xenograft PAC tumors in mice (1). The TF10 bsmAb is divalent for binding to MUC1 and monovalent for binding to a histamine-succinyl-glycine (HSG) motif containing hapten (DOTA-D-Tyr-D-Lys(HSG)-D-Glu-D-Lys(HSG)-NH_2_; IMP-288; HSG hapten), which was generated by linking two PAM4 Fab fragments to an anti-HSG hapten mAb Fab fragment as described elsewhere (1). Recently, the use of ^90^Y-labeled IMP-288 in the pretargeted radioimmunotherapy of mice bearing PAC tumors was shown to be superior to the application of ^90^Y-labeled PAM4 IgG alone in the animals (11). The biodistribution of ^111^In-labeled IMP-288 ([^111^In]-IMP-288) and the visualization of PAC tumors in mice with this labeled hapten is discussed in this chapter. The biodistribution of ^125^I-labeled TF10 ([^125^I]-TF10) was studied in mice bearing PAC tumors and is discussed in a separate chapter of MICAD (www.micad.nih.gov) (12).

### Related Resource Links

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-TF10%20synthesis&cmd=DetailsSearch)]

IMP-288 was obtained from a commercial source and labeled with ^111^In as described elsewhere (1). PAM4 IgG was also labeled with ^111^In for use as a control as described by Gold et al. (1). The specific activities of [^111^In]-IMP-288 and [^111^In]-PAM4 IgG were 222 kBq/pmol (6 μCi/pmol) and 15.2 kBq/pmol (0.41 μCi/pmol), respectively. The purity of these labeled compounds was determined with size-exclusion high-performance liquid chromatography and instant thin-layer chromatography. The purity and yield of the radiolabeled compound was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10&cmd=DetailsSearch)]

Size-exclusion chromatography analysis of a [^111^In]-IMP-288/TF10 mixture showed that 90% of the labeled peptide was bound to the trivalent bsmAb (1). When the labeled hapten was exposed to TF10 in the presence of excess MUC1, 92% eluted at a higher molecular weight, 3% eluted in the non-MUC1 reactive TF10 fraction, and 5% remained as free hapten. [^111^In]-IMP-288 did not bind MUC1 in the absence of TF10.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-IMP-288 was investigated in athymic nude mice bearing subcutaneous human xenograft pancreatic adenocarcinoma CaPan-1 cell tumors pretargeted with TF10 in a bsmAb/labeled hapten (b/h) ratio of 10:1 (1). One group of animals (n = 5 mice/group) was injected with 80 μg TF10, and a second group (control) was left untreated. At 16 h postinjection (p.i.), the animals were injected with 30 μCi [^111^In]-IMP-288, and the mice were euthanized at various time points to determine the amount of radioactivity taken up by the organs of interest, including tumors. Results were presented as a percent of injected dose per gram tissue (% ID/g). For comparison, another group of mice was injected with [^111^In]-PAM4 IgG and treated as described above (1).

At 3 h p.i., most of the radioactivity had cleared from blood (0.01% ID/g), and all tissues had an uptake between ~0.02% ID/g (normal pancreas and stomach) and 1.72 ± 0.24% ID/g (kidneys). With a b/h ratio of 10:1, the tumors showed an accumulation of 24.3 ± 1.17% ID/g at this time point; with a b/h ratio of 20:1, the tumor uptake increased to 28.6 ± 0.73% ID/g, whereas no increase in uptake was observed in the other tissues. The tumor/blood and tumor/pancreas ratios were ~1,000 and ~900, respectively, but for other tissues this ratio was usually ~100. No blocking studies were reported.

Scintigraphic images were acquired at 3 h p.i. from animals pretargeted with TF10 and then treated with the labeled hapten (b/h ratio 10:1) (1). Another group of animals was injected with the radiolabeled hapten alone. Images acquired from the pretargeted animals showed a very high concentration of radioactivity in the tumors, but no lesions were visible in mice that were treated with [^111^In]-IMP-288 alone. By comparison, the tumors were visible only at 24 h p.i. in animals injected with [^111^In]-PAM4 IgG, and the accumulation of label in the lesions peaked at 48 h p.i. The investigators did not report any study confirming the binding specificity of [^111^In]-IMP-288 to TF10.

From these studies, the investigators concluded that superior images were generated with [^111^In]-IMP-288 when tumors in the mice were pretargeted with TF10 compared to using [^111^In]-PAM4 IgG alone (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by National Cancer Institute, National Institutes of Health, grants CA096924 and CA115755.

## References

1 Gold D.V., et al. (2008). A novel bispecific, trivalent antibody construct for targeting pancreatic carcinoma. Cancer Res.
2 Gold D.V., et al. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
3 Gold D.V., et al. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
4 Cardillo T.M., et al. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.
5 Ahlgren S., et al. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
6 Forster G.J., et al. (2006). Pretargeted radioimmunotherapy with a single-chain antibody/streptavidin construct and radiolabeled DOTA-biotin: strategies for reduction of the renal dose. J Nucl Med.
7 Liu G., et al. (2010). Tumor pretargeting in mice using MORF conjugated CC49 antibody and radiolabeled complimentary cMORF effector. Q J Nucl Med Mol Imaging.
8 Uppal J.K., et al. (2011). Biological evaluation of avidin-based tumor pretargeting with DOTA-Triazole-Biotin constructed via versatile Cu(I) catalyzed click chemistry. J Drug Target.
9 Goldenberg D.M., Sharkey R.M. (2010). Radioactive antibodies: a historical review of selective targeting and treatment of cancer. Hosp Pract (Minneap).
10 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
11 Karacay H., et al. (2009). Pretargeted radioimmunotherapy of pancreatic cancer xenografts: TF10-90Y-IMP-288 alone and combined with gemcitabine. J Nucl Med.
12 Chopra, A., 125I-Labeled trivalent, bispecific monoclonal antibody construct TF10 that targets mucin-1 and is reactive against a histamine-succinyl-glycine hapten IMP-288. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.